# LLP2A-biotin-streptavidin-Alexa Fluor 680

Chemical name: | LLP2A-biotin-streptavidin-Alexa Fluor 680
Abbreviated name: | LLP2A-SA-Alexa680
Synonym:
Agent Category: | Peptide
Target: | Integrin α_4_β_1_
Target Category: | Receptor binding
Method of detection: | Optical, near-infrared fluorescence
Source of signal: | Alexa Fluor 680 (Alexa680)
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=119631392), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=67191026) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3676) for more information about integrin α_4_β_1_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A)]

Optical fluorescence imaging is increasingly being used to observe biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

Integrins are a family of cell-surface heterodimeric glycoproteins that mediate diverse biological events involving cell–cell and cell–matrix interactions (3). They consist of an α and a β subunit, and they are important for cell adhesion and signal transduction. The α_4_β_1_ integrin plays an important role in hematopoiesis of lymphocytes; on the other hand, the α_4_β_1_ integrin affects tumor growth, tumor invasiveness, and metastasis (4). The α_4_β_1_ integrin is strongly expressed on lymphoid tumor cells (5). LLP2A was identified as a peptidomimetic ligand to bind to α_4_β_1_ integrin on human Jurkat T-lymphoid leukemia cells using “one-bead one-compound” combinatorial libraries (6). LLP2A was conjugated with Alexa Fluor 680 (Alexa680) via biotin and streptavidin (SA) interaction to study in vivo biodistribution of the tracer in tumor-bearing mice. Alexa680 is a NIR fluorescent dye with an absorbance maximum at 684 nm and an emission maximum at 707 nm with a high extinction coefficient of 183,000 (mol/L)^-1^cm^-1^. LLP2A-biotin-SA-Alexa680 was found to have a high specific accumulation in α_4_β_1_-positve lymphoid tumor cells in nude mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+synthesis)]

LLP2A and LLP2A-biotin were obtained using solid-phase synthesis (6). LLP2A-biotin was coupled to Alexa680-SA by use of the strong interaction between biotin and SA to form LLP2A-SA-Alexa680.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+and+in+vitro)]

LLP2A exhibited a 50% inhibition concentration of 2.0 ± 1.4 pM in a cell-based, α_4_β_1_-mediated adhesion assay using Jurkat cells with a linear peptide (25 amino acids) of fibronectin (6). LLP2A was stable in human plasma for up to 18 days at 37°C. Flow cytometry and fluorescent microscopy confirmed the binding of LLP2A-biotin to α_4_β_1_-positive cells (Jurkat and Molt-4 leukemia cells) and not to α_4_β_1_-negative cells (A549 lung cancer cells). The binding to Molt-4 cells was inhibited by either LLP2A or anti-α_4_ monoclonal antibody HP2/1. Furthermore, LLP2A-biotin did not bind to cell lines transfected with α_2_β_1_, α_5_β_1_, α_6_β_1_, α_9_β_1_ (closely related to α_4_β_1_), α_L_β_2_, or α_M_β_1_, which indicated that LLP2A is specific to α_4_β_1_. LLP2A-biotin exhibited strong binding to Jurkat leukemia cells but weak binding to normal lymphocytes.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+rodentia)]

Peng et al. (6) performed biodistribution studies of LLP2A-SA-Alexa680 in nude mice bearing a Molt-4 subcutaneous xenograft. Images were obtained after injection of 60 nmol/kg of LLP2A-SA-Alexa680. Substantial contrasts were observed between the Molt-4 tumor and normal tissue from 6 h until 44 h with a maximal difference at 24 h. Pretreatment with anti-α_4_ monoclonal antibody HP2/1 reduced fluorescent uptake into the tumor. Negligible fluorescence uptake into the tumor was observed with injection of SA-Alexa680 or scrambled LLP2A-SA-Alexa680. Ex vivo imaging showed that most of the LLP2A-SA-Alexa680 fluorescent signal intensity was seen in the Molt-4 tumors and kidneys. Cellular fluorescence was also observed in some blood vessels within the Molt-4 tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+human)]

No publication is currently available.

## NIH Support

R33 CA86364, R33 CA99136, U19 CA113298

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Hynes R.O., Lively J.C., McCarty J.H., Taverna D., Francis S.E., Hodivala-Dilke K., Xiao Q. (2002). The diverse roles of integrins and their ligands in angiogenesis. Cold Spring Harb Symp Quant Biol.
4 Holzmann B., Gosslar U., Bittner M. (1998). alpha 4 integrins and tumor metastasis. Curr Top Microbiol Immunol.
5 Vincent A.M., Cawley J.C., Burthem J. (1996). Integrin function in chronic lymphocytic leukemia. Blood.
6 Peng L., Liu R., Marik J., Wang X., Takada Y., Lam K.S. (2006). Combinatorial chemistry identifies high-affinity peptidomimetics against alpha4beta1 integrin for in vivo tumor imaging. Nat Chem Biol.